# 1-(2'-Deoxy-2'-[^18^F]fluoroarabinofuranosyl)cytosine

Chemical name: | 1-(2'-Deoxy-2'-[^18^F]fluoroarabinofuranosyl)cytosine
Abbreviated name: | [^18^F]FAC
Synonym:
Agent category: | Compound
Target: | Deoxycytidine kinase (DCK)
Target category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FAC)]

One of the characteristics of tumor cells is their unchecked proliferation. It is important to measure the proliferation rate of cancer lesions to help differentiate benign tumors from malignant tumors and to characterize malignant tumors among normal tissues. 2-[^18^F]Fluoro-2-deoxy-D-glucose ([^18^F]FDG (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=FDG)) has been approved (http://www.fda.gov/Drugs/DevelopmentApprovalProcess/Manufacturing/ucm182642.htm) for cancer positron emission tomography (PET) imaging by the United States Food and Drug Administration. However, enhanced uptake of FDG as measurement of glycolysis occurs in inflammatory cells and lesions as well as in necrotic cells (1, 2). Thymidine (TdR) and TdR analogs are the standard markers for DNA synthesis, and [^11^C]TdR has been used in PET to measure tumor growth rates in situ. Because of the short half-life of ^11^C and the extensive metabolism of [^11^C]TdR in the blood (3), 3'-deoxy-3'-[^18^F]fluorothymidine (FLT (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=Fluorothymidine18F)) was developed for PET imaging. FLT is an analog of TdR and is phosphorylated by TdR kinase-1 (TK-1), an enzyme expressed during the DNA synthesis phase (S-phase) of the cell cycle (4). On the other hand, RNA synthesis occurs in all phases of the cell cycle except the M phase, even in slow-growing solid tumors. Tracers targeted to RNA synthesis could be used to visualize tumors with low TK-1 expression.

Phosphorylation of deoxyribonucleosides and their nucleoside analogs is carried out with deoxycytidine kinase (DCK) (5). DCK is ubiquitously expressed in normal tissues but is highly expressed in hematolymphoid tissues (spleen, thymus, and lymph nodes) and epithelial cells (6). Lymphoid cells and rapidly proliferating cells prefer the salvage pathway over the de novo pathway for DNA synthesis. 1-(2'-Deoxy-2'-fluoroarabinofuranosyl)cytosine (FAC) was found to be retained in proliferating T cells. FAC is taken up by cells and rapidly phosphorylated by DCK and trapped inside the cells. In this chapter, 1-(2'-deoxy-2'-[^18^F]fluoroarabinofuranosyl)cytosine ([^18^F]FAC) is being developed as a PET probe for imaging of epithelium, lymphoid tissues, and immune activation (6-8).

### Related Resource Links:

- Chapters in MICAD (Nucleoside (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=nucleoside%20+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (DCK (http://www.ncbi.nlm.nih.gov/gene/1633))
- Articles in Online Mendelian Inheritance in Man (OMIM) (DCK (http://www.ncbi.nlm.nih.gov/omim/125450))
- Clinical trials ([^18^F]FAC (http://www.clinicaltrials.gov/ct2/results?term=L-FAC))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FAC%20and%20synthesis)]

Radu et al. (8) reported the synthesis of [^18^F]FAC using 1-bromo-2-[^18^F]fluoro-3,5-di-O-benzoyl-D-arabinofuranose sugar derivative. [^18^F]FAC was purified with high-performance liquid chromatography with a radiochemical purity of >99% and radiochemical yields of 20%–30%. The specific activity of [^18^F]FAC was >37 GBq/µmol (1 Ci/µmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FAC%20and%20in%20vitro)]

In vitro cellular uptake assays with murine lymphoid cells from the thymus and spleen showed that CD8^+^ T cells and CD11b^+^ cells (macrophages and granulocytes) exhibited higher uptake of [^18^F]FAC than did CD4^+^ T cells (8). Activated mouse CD8^+^ T cells (250 fmol/10^5^ cells) showed >12-fold higher uptake of [^3^H]FAC than did resting CD8^+^ T cells (18 fmol/10^5^ cells). NIH3T3 fibroblasts transfected with DCK and solute carrier family SLC29A1 genes showed ~1–2-fold higher uptake of [^3^H]FAC than did control cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FAC%20and%20rodentia)]

Radu et al. (8) performed ex vivo biodistribution studies after injection of 7.4 MBq (200 μCi) [^18^F]FAC in normal mice (n = 3). The radioactivity at 60 min after injection was highest in the urinary bladder (35% injected dose/gram (ID/g)), followed by the spleen (9% ID/g), thymus (7% ID/g), lymph nodes (5% ID/g), small intestine (5% ID/g), and large intestine (4% ID/g). The accumulation in the heart, kidney, lung, liver, and muscle was <4% ID/g. Whole-body PET imaging visualized [^18^F]FAC accumulation in the thymus, spleen, intestines, liver, bone, and bone marrow at 60 min after injection. Fractionations of the cells from the thymus and spleen showed that the thymocytes, T cells, B cells, macrophages, and granulocytes had high accumulation of radioactivity. Analysis of thymus extract showed that [^18^F]FAC and its phosphorylated derivatives (mono-, di-, and tri-phosphate metabolites) were detected at 60 min after injection. As a comparison, the spleen showed higher accumulation of [^18^F]FAC (2.16 ± 0.48% ID/g) than of [^18^F]FLT (1.02 ± 0.21% ID/g) or [^18^F]FDG (1.69 ± 0.16% ID/g). [^18^F]FAC PET imaging studies in a mouse model of antitumor immunity clearly visualized activated lymphoid organs (spleen and tumor-draining lymph nodes). Splenic CD8^+^ T cells exhibited three-fold higher [^18^F]FAC accumulation compared with naïve T cells. In a systemic autoimmunity model, PET imaging revealed increased numbers of [^18^F]FAC-positive lymph nodes in B6.MRL-Fas^lpr^ autoimmune mice as compared with wild-type mice. Administration of 10 mg/kg dexamethasone (an immunosuppressive drug) decreased the numbers of [^18^F]FAC-positive lymph nodes in B6.MRL-Fas^lpr^ mice.

Brewer et al. (6) demonstrated that the high uptake of [^18^F]FAC in the intestines in normal mice was mainly contributed by the epithelial cells, with some contribution from T cells. Germ-free mice showed lower uptake in the intestine, whereas mice with immune inflammatory stimulation (transfer of T cells from colitic mice) showed higher uptake than the normal mice.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FAC%20and%20(dog%20or%20pig%20or%20sheep%20or%20rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FAC%20and%20(primate%20not%20human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20FAC%20and%20human)]

No publication is currently available.

## NIH Support

P50 CA86306, 5U54 CA119347

## References

1 Kubota R., Yamada S., Kubota K., Ishiwata K., Tamahashi N., Ido T. (1992). Intratumoral distribution of fluorine-18-fluorodeoxyglucose in vivo: high accumulation in macrophages and granulation tissues studied by microautoradiography. J Nucl Med.
2 van Waarde A., Cobben D.C., Suurmeijer A.J., Maas B., Vaalburg W., de Vries E.F., Jager P.L., Hoekstra H.J., Elsinga P.H. (2004). Selectivity of 18F-FLT and 18F-FDG for differentiating tumor from inflammation in a rodent model. J Nucl Med.
3 Ishiwata K., Ido T., Abe Y., Matsuzawa T., Murakami M. (1985). Studies on 18F-labeled pyrimidines III. Biochemical investigation of 18F-labeled pyrimidines and comparison with 3H-deoxythymidine in tumor-bearing rats and mice. Eur J Nucl Med.
4 Sherley J.L., Kelly T.J. (1988). Regulation of human thymidine kinase during the cell cycle. J Biol Chem.
5 Arner E.S., Eriksson S. (1995). Mammalian deoxyribonucleoside kinases. Pharmacol Ther.
6 Brewer S., Nair-Gill E., Wei B., Chen L., Li X., Riedinger M., Campbell D.O., Wiltzius S., Satyamurthy N., Phelps M.E., Radu C., Witte O.N., Braun J. (2010). Epithelial uptake of [18F]1-(2'-deoxy-2'-arabinofuranosyl) cytosine indicates intestinal inflammation in mice. Gastroenterology.
7 Nair-Gill E., Wiltzius S.M., Wei X.X., Cheng D., Riedinger M., Radu C.G., Witte O.N. (2010). PET probes for distinct metabolic pathways have different cell specificities during immune responses in mice. J Clin Invest.
8 Radu C.G., Shu C.J., Nair-Gill E., Shelly S.M., Barrio J.R., Satyamurthy N., Phelps M.E., Witte O.N. (2008). Molecular imaging of lymphoid organs and immune activation by positron emission tomography with a new [18F]-labeled 2'-deoxycytidine analog. Nat Med.